# Cy5-Glu-Pro-Asp-acyloxymethyl ketone

Chemical name: | Cy5-Glu-Pro-Asp-acyloxymethyl ketone
Abbreviated name: | Cy5-AB50
Synonym:
Agent category: | Compound
Target: | Caspase-3, caspase-7
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Caspase%20ABPs)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (3). Apoptosis is gene-regulated (4) and is the result of proteolysis of intracellular components by activation of a series of proteolytic enzymes called caspases preceding changes in the plasma membrane structure by translocase, floppase, and scramblase (5-7). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein produced in particular by epithelial cells in many tissues, such as the placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (8). Annexin V binds to PS with high affinity (K_D_ = 7 nM) (5, 9, 10). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathological conditions (7); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^18^F, ^123^I, ^125^I, and ^99m^Tc for imaging (11-14). However, annexin V is not able to distinguish between apoptosis and necrosis. The caspase ligand may be an attractive alternative for imaging cells undergoing apoptosis because caspases are key enzymes that mediate apoptosis (15). Berger et al. (16) reported that acyloxymethyl ketone peptides exhibited selective inhibition of caspase-3 and caspase-7 (executioner caspases) over caspase-8 and caspase-9 (initiator caspases). Glu-Pro-Asp-acyloxymethyl ketone (EPD-AOMK or AB50) has been conjugated with Cy5 for NIR imaging of caspase-3/7 activation in apoptosis (17).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Caspase+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Caspase-3 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=836), Caspase-7 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=840)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=GRPR)
- Clinical trials (Caspase inhibitors (http://www.clinicaltrials.gov/ct2/results?term=caspase+inhibitor))
- Drug information in FDA (http://google2.fda.gov/search?q=caspase+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=14)
- Information about Cy5-AB50 in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=search&db=pcsubstance&term=85752741)
- Information about caspase inhibitors in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pcsubstance&Cmd=DetailsSearch&Term=caspase%5BAll+Fields%5D+AND+inhibitor%5BAll+Fields%5D)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Caspase%20ABPs%20and%20synthesis)]

AB50 was synthesized with the solid-phase synthesis method (17). Cy5 was coupled to AB50 to form Cy5-AB50 using the methods as reported by Blum et al. (18). Cy5-AB50 was purified with column chromatography. The identity of Cy5-AB50 was confirmed with liquid chromatography mass spectroscopy with one Cy5 per molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Caspase%20ABPs+and+in+vitro)]

In vitro caspase enzyme assays using AB50 showed inhibition concentration value of ~8 nM for caspase-3 in competition with Cy5-AB46 (17). Induction of caspase-3/7 apoptosis with anti-Fas antibodies in Jurkat tumor cells increased accumulation of Cy5-AB50 (100 nM) over the untreated cells at 30 min and 120 min. The increased caspase activities were completely blocked with AB50 pretreatment. Cy5-AB50 did not bind to cathepsin B as expected.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Caspase%20ABPs%20and%20rodentia)]

Edgington et al. (17) performed ex vivo accumulation studies in the thymus in mice treated with dexamethasone for 6, 12, or 24 h (n = 3 mice per group). The thymi were excised for analysis at 2 h after injection of Cy5-AB50 (50 nmol). Caspase-3/7 activity was visualized at 6 h (~12 arbitrary units (au)) after injection, peaked at 12 h (~40 au), and returned to background level at 24 h (~8 au) after injection. The amount of caspase-3/7 in the thymi was confirmed with immunoprecipitation. NIR imaging was performed in tumor-bearing mice treated with Apomab (a DR5-targeted pro-apoptotic receptor agonist) for 2, 5, 8, 11, and 17 h to induce apoptosis in the tumors (19). Tumor fluorescence signal was monitored at 1 h after injection of Cy5-AB50. Quantification of total tumor fluorescence signal correlated with caspase-3/7 levels as measured with gel analysis. The tumor fluorescence peaked at 12 h with more than three-fold increase over the background at 0 h. Whole-body NIR imaging at 12 h showed that there was a four-fold increase of tumor fluorescence intensity in mice treated with Apomab as compared with mice treated with vehicle. No blocking experiment was performed. Quantitation of the % ID/g was not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Caspase%20ABPs%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Caspase%20ABPs%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Caspase%20ABPs%20and%20human)]

No publications are currently available.

## NIH Support

P01 CA072006, CA09302, R01 EB005011, U54 RR020843

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
4 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
5 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
6 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
7 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
8 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
9 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
10 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
11 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
12 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
13 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
14 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
15 Neuss M., Crow M.T., Chesley A., Lakatta E.G. (2001). Apoptosis in cardiac disease--what is it--how does it occur. Cardiovasc Drugs Ther.
16 Berger A.B., Witte M.D., Denault J.B., Sadaghiani A.M., Sexton K.M., Salvesen G.S., Bogyo M. (2006). Identification of early intermediates of caspase activation using selective inhibitors and activity-based probes. Mol Cell.
17 Edgington L.E., Berger A.B., Blum G., Albrow V.E., Paulick M.G., Lineberry N., Bogyo M. (2009). Noninvasive optical imaging of apoptosis by caspase-targeted activity-based probes. Nat Med.
18 Blum G., von Degenfeld G., Merchant M.J., Blau H.M., Bogyo M. (2007). Noninvasive optical imaging of cysteine protease activity using fluorescently quenched activity-based probes. Nat Chem Biol.
19 Zinonos I., Labrinidis A., Lee M., Liapis V., Hay S., Ponomarev V., Diamond P., Zannettino A.C., Findlay D.M., Evdokiou A. (2009). Apomab, a fully human agonistic antibody to DR5, exhibits potent antitumor activity against primary and metastatic breast cancer. Mol Cancer Ther.